# trans-(+)-1,2,3,5,6,10b-Hexahydro-6-(4-([^11^C]methylthio)-phenyl)pyrrolo-(2,1-a)-isoquinoline

Chemical name: | trans-(+)1,2,3,5,6,10b-Hexahydro-6-(4-([^11^C]methylthio)-phenyl)pyrrolo-(2,1-a)-isoquinoline
Abbreviated name: | [^11^C](+)McN5652; [^11^C]McN5652
Synonym:
Agent Category: | Compound
Target: | Serotonin transporter (SERT); 5-HT
Target Category: | Ligand binding
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Other non-primate mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=McN5652%5BAll%20Fields%5D)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?CMD=search&DB=pubmed]

The neurotransmitter serotonin (5-HT) plays a major role in a variety of brain functions, such as appetite, sleep, and mood. Neuropsychiatric disorders, including major depression, schizophrenia, Alzheimer’s disease, and Parkinson’s disease (1-3), involve a dysfunction of the brain’s 5-HT system.

The serotonergic neurons – present in wide areas of the brain, including the raphe nuclei, hypothalamus, thalamus, and cerebral cortex – bear a protein called “serotonin transporter” (SERT) (4).The SERT, located on the cell bodies and terminals of 5-HT neurons, is a specific marker for the number and integrity of presynaptic terminals of serotonin-producing neurons. It regulates neurotransmission by removing released 5-HT from the extracellular space back into the presynaptic neuron. Commonly prescribed antidepressants are selective serotonin reuptake inhibitors, and their effects are obtained through interaction with (and inhibition of) the SERT (5). For that reason, in vivo imaging of the regional brain distribution of the SERT is an important tool for studying the 5-HT system and the treatment of neuropsychiatric disorders.

A variety of in vivo radioligands for positron emission tomography (PET) have been evaluated for imaging the SERT. trans-(+)1,2,3,5,6,10b-Hexahydro-6-(4-([^11^C]methylthio)-phenyl)pyrrolo-(2,1-a)-isoquinoline ([^11^C]McN5652) was the first successful and widely used agent (6, 7). However, it does have some limitations; for example, its kinetics in the brain are slow, and although adequate for regions with high SERT density, it often provides insufficient signal-to-noise differentials for imaging brain regions with intermediate to low SERT densities (e.g., limbic and neocortical regions) because of its high nonspecific binding. Over recent years, new PET radioligands have been synthesized and evaluated as SERT imaging agents and alternatives to [^11^C]McN5652 (e.g [^11^C]DASB, [^11^C]AFM, [^11^C]ADAM, [^11^C]HOMADAM).

[^11^C]McN5652 has two optical isomeric forms. The ability of its geometric trans (+), pharmacologically active enantiomer, [^11^C](+)McN5652, to block the SERT is at least two orders of magnitude higher than that of its inactive enantiomer, [^11^C](-)McN5652 (8, 9) (inhibition constant (K_i_) ~ 0.7 nM for [^11^C](+)McN5652 versus 0.4 nM for [^11^C](-)McN5652) (also see the In Vitro Studies section). Brain uptake and retention of [^11^C](+)McN5652 correspond to the distribution of the SERT in rodents, non-human primates, and humans. Several methods have been used to quantify [^11^C](+)McN5652-specific binding, but the high level of nonspecific binding, the differences in nonspecific binding among regions, and the slow equilibration between specific and nonspecific binding populations have made such a quantification difficult (10).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=McN5652%5BAll%20Fields%5D%20AND%20synthesis)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoroflumazenil%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D]

In 1995, Suehiro et al. (11) reported details of a synthetic procedure for [^11^C]McN5652 that addressed the instability issue of the thiol precursor used in previous established synthesis methods (12). This improved procedure involved the saponification of thioesters and enabled reaction of the precursor of McN5652 in a one-pot radiolabeling sequence. After hydrolysis of the thioester functionality (via tetrabutylammonium hydroxide for 10 min), the free thiol was reacted in situ with [^11^C]iodomethane (in dimethyl formamide, at 40-45 °C, for 1 min) without purification. The radiolabeled material produced was stable and could be used for multiple experiments.

The radiochemical yield obtained for [^11^C]McN5652 was ~26% (decay-corrected at end of bombardment), and the total synthesis time, as reported by Suehiro et al. (11), was about 18 min. The specific activity of the radiotracer produced was ~84,730 MBq/μmol (2,290 mCi/μmol).

Details of a synthetic method for [^11^C](+)McN5652 by S-methylation of the corresponding precursor with [^11^C]iodomethane using an automated process were reported by Sasaki et al. (13). In this method, the desmethyl precursor was obtained by demethylation of nonradioactive McN5652 and successive stabilization by the addition of dithiothreitol (DTT), a protecting agent for the SH group, immediately after reaction. This method led to a radiochemical purity of 98.6 ± 0.4% and specific activity for [^11^C](+)McN5652 of 181.3 ± 7.4 GBq/μmol (4,900 ± 200 mCi/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=McN5652%5BAll%20Fields%5D%20AND%20in%20vitro%5BAll%20Fields%5D)]

In vitro inhibition studies performed by Shank et al. (9) showed that (+)McN5652 had the ability to prevent 5-HT uptake to a much greater extent than norepinephrine, whereas its potency for dopamine uptake was negligible. Its inhibition constant was found to be in the nanomolar range (K_i_ = 0.40 nM for synaptosomal 5-HT uptake), which was similar to those of paroxetine and sertraline, two high-affinity ligands for 5-HT. The optically inactive McN5652 enantiomer exhibited a much lower affinity (~150 lower) for the SERT than its optically active isomer (9).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=McN5652%20AND%20%22rodentia%22%5BMeSH%20Terms%5D)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HOMADAM%20AND%20%22rodentia%22]

Mice studies performed by Suehiro et al. (7) showed that [^11^C](+)McN5652 had a higher uptake and longer retention in regions with high density of 5-HT uptake sites than the ^11^C-labeled racemic mixture and that [^11^C](-)McN5652 washed out rapidly. With the trans form [^11^C](+) enantiomer, the hypothalamus/cerebellum ratio reached 6 at 90 min. When mice received injections of the selective 5-HT uptake blocker paroxetine (5 mg/kg of tissue) before injections of [^11^C](+)McN5652, binding of [^11^C](+)McN5652 was inhibited by 45 to 73% in all regions except in the cerebellum. [^11^C](-)McN5652 showed no specific binding in any of the regions.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=McN5652%20AND%20%28dog%20OR%20pig%20OR%20sheep%29)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HOMADAM%20AND%20%28dog%20OR%20sheep%20OR%20pig%29]

Brust et al. (14) performed comparative studies between [^11^C]McN5652 and its analog S-([^18^F]fluoromethyl)-(+)-McN5652 in 6-week-old female pigs. The animals received an infusion of the radiotracers (over 2 min into the jugular vein) at the following doses: 242 ± 94 GBq/μmol (6,540 ± 2,540 mCi/μmol) for [^11^C](+)McN5652 and 274 ± 110 GBq/μmol (7,405 ± 2,973 mCi/μmol) for S-([^18^F]fluoromethyl)McN5652. PET scans showed that the highest accumulation of both radiotracers was in the ventral midbrain, thalamus, olfactory lobe, and pons, consistent with the known densities of 5-HT transporters. In addition, the kinetics of S-([^18^F]fluoromethyl)-(+)-McN5652 appeared to be faster. A peak of activity in the midbrain was reached at ~12 min post injection, whereas the maximum radioactivity was reached at ~22 min post injection for [^11^C](+)McN5652. Strong inhibition of the specific binding was observed for both radiotracers after pretreatment with the selective 5-HT uptake inhibitor citalopram (5 mg/kg of tissue).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=McN5652%20AND%20%28primate%20NOT%20human%29)]

Szabo et al. (15) performed dynamic PET scans using [^11^C]McN5652 on 3 Papio anubis baboons. The animals first received injections of [^11^C](+)McN5652, followed by the pharmacologically inactive enantiomer [^11^C](-)McN5652 (specific activities at time of injection: 64,195 ± 21,645 MBq/μmol (1,735 ± 585 mCi/μmol) for the (+) enantiomer and 93,721 ± 42,661 MBq/μmol (2,533 ± 1,153 mCi/μmol) for the (-) enantiomer); two animals received [^11^C](+)McN5652 after pretreatment with the specific 5-HT uptake site inhibitor fluoxetine (5 mg/kg of tissue).

Results showed that the initial brain uptake into the brain was similar for both [^11^C](+)McN5652 and [^11^C](-)McN5652, but that at later times (45-120 min after injection), only [^11^C](+)McN5652 exhibited a distribution pattern characteristic for 5-HT uptake sites (prominent uptake in the midbrain, hypothalamus, striatum, and pons; medium uptake in the cerebral cortex; and minimal activity in the cerebellum). On the other hand, in studies with [^11^C](-)McN5652 and with [^11^C](+)McN5652 after 5-HT uptake site blockade with fluoxetine, the radiotracer uptakes were significantly lower and the distribution pattern was relatively even. The differences between [^11^C](+)McN5652 and [^11^C](-)McN5652 were calculated for the time interval 95-125 min post injection and used to estimate specific binding. Specific binding correlated well with the known density of 5-HT uptake sites (r = 0.95; P < 0.001) in the human brain, as determined in vitro by Laruelle and Maloteaux (16). There was also a high correlation (r = 0.81; P < 0.002) between specific binding obtained with [^11^C](+)McN5652 (or [^11^C](-)McN5652) and that obtained with blockade by fluoxetine. At 95-125 min post injection, the midbrain/cerebellum ratio obtained for [^11^C](+)McN5652 was 1.50 ± 0.38 without fluoxetine and 0.91 ± 0.16 with fluoxetine.

Other primate PET studies using both [^11^C](+)McN5652 and [^11^C](-)McN5652 were performed by Kakiuchi et al. (17). The aim of the studies was to investigate age-related changes in the SERT for living brains of conscious young (5.9 ± 1.8 years old) and aged (19.0 ± 3.3 years old) Macaca mulatta monkeys. Results showed that specific binding of the SERT was higher in the thalamus and striatum, with intermediate binding in the pons, hippocampus, cingulate gyrus, and cortical regions, and lower binding in the cerebellum (in both young and aged monkeys). Almost all regions – except the cerebellum – showed significant age-related decreases in specific binding of the SERT. When the SERT blocker fluvoxamine (1 mg/kg of tissue) was administered intravenously at 30 min after injection of the radiotracer, the specific binding of the SERT was displaced in both age groups.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=McN5652%20AND%20human)]

The first studies of the serotonin 5-HT transporter in the living human brain, using PET with [^11^C](+)McN5652, were reported by Szabo et al. (18). The experimental protocol involved injecting either [^11^C](+)McN5652 or [^11^C](-)McN5652 into three healthy subjects, and in two cases, injecting [^11^C](+)McN5652 after pretreatment with the 5-HT uptake site blocker fluoxetine. Results showed highest accumulation of [^11^C](+)McN5652, with a steady increase over 120 min after injection of the radiotracer. In contrast, with [^11^C](-)McN5652 and when [^11^C](+)McN5652 binding was inhibited with fluoxetine, radioactivity concentrations declined after reaching a peak at 20 to 30 min post injection.

Reivich et al. (19) used [^11^C](+)McN5652 as a PET agent to study alterations in the brain 5-HT system in patients with depression. In their experiments, four drug-free depressed patients and four healthy control subjects received intravenous injections containing 7-10 mCi of [^11^C](+)McN5652, and 18 sequential PET scans were obtained at increasing time periods. Distribution volume (DV) ratios of [^11^C](+)McN5652 (compared with the cerebellum) were calculated in selected regions of interest, using a two-compartment model (20). Results showed significantly larger DV ratios in the left frontal cortex (P = 0.013) and the right cingulate cortex (P = 0.043), compared with healthy controls. Mean region/cerebellum DV ratios were as follows: 1.941 (in patients) and 1.667 (in control subjects) for the right thalamus, 1.678 (patients) and 1.153 (controls) for the right pons, and 1.359 (patients) and 1.092 (controls) for the right cingulate.

PET studies comparing [^11^C](+)McN5652 and [^11^C]cyanoimipramine were performed by Takano et al. (21) in 15 healthy volunteers. [^11^C](+)McN5652 was injected at a dose of 179-759 MBq (4.8-20.5 mCi), and [^11^C]cyanoimipramine was injected at a dose of 360-721 MBq before PET scans were performed. The following mean thalamus/cerebellum, striatum/cerebellum, and frontal cortex/cerebellum ratios were obtained at 90 min post injection: 1.61 ± 0.15, 1.59 ± 0.10, and 1.08 ± 0.07 for [^11^C](+)McN5652 and 1.72 ± 0.18, 1.72 ± 0.18, and 1.17 ± 0.12 for [^11^C]cyanoimipramine. After pretreatment with 50 mg of clomipramine (injected dose, 370 MBq (100 mCi)), the DVs of [^11^C](+)McN5652 in the cerebellum and frontal cortex were not significantly changed, but those in the thalamus and striatum were dramatically decreased. The mean thalamus/cerebellum, striatum/cerebellum, and frontal cortex/cerebellum ratios for [^11^C](+)McN5652 obtained at 90 min post injection were 1.20 ± 0.06, 1.31 ± 0.05, and 0.98 ± 0.03, respectively.

Over recent years, a number of human PET studies using [^11^C](+)McN5652 have been performed to evaluate the neurotoxic effects of (±)3,4-methylenedioxymethamphetamine (MDMA; “ecstasy”) on human brain 5-HT system (22-24). In a study by McCann et al (23). using [^11^C](+)McN5652 and [^11^C]DASB, global reductions in SERT concentrations were found in MDMA users with both PET ligands. [^11^C](+)McN5652 has also been used in PET studies for quantifying the SERT in patients with bipolar disorder (21) and social phobia (25).

## References

1 Owens MJ Nemeroff CB The serotonin transporter and depression Depress Anxiety 1998 8Suppl 15 12 9809208
2 Palmer AM, Francis PT, Benton JS, Sims NR, Mann DM, Neary D, Snowden JS, Bowen DM. (1987). Presynaptic serotonergic dysfunction in patients with Alzheimer's disease. J Neurochem.
3 Roth BL, Xia Z. (2004). Molecular and cellular mechanisms for the polarized sorting of serotonin receptors: relevance for genesis and treatment of psychosis. Crit Rev Neurobiol.
4 Laakso A, Hietala J. (2000). PET studies of brain monoamine transporters. Curr Pharm Des.
5 White KJ, Walline CC, Barker EL. (2005). Serotonin transporters: implications for antidepressant drug development. Aaps J.
6 Ichimiya T, Suhara T, Sudo Y, Okubo Y, Nakayama K, Nankai M, Inoue M, Yasuno F, Takano A, Maeda J, Shibuya H. (2002). Serotonin transporter binding in patients with mood disorders: a PET study with [11C](+)McN5652. Biol Psychiatry.
7 Suehiro M, Scheffel U, Ravert HT, Dannals RF, Wagner HN. (1993). [11C](+)McN5652 as a radiotracer for imaging serotonin uptake sites with PET. Life Sci.
8 Szabo Z, Scheffel U, Mathews WB, Ravert HT, Szabo K, Kraut M, Palmon S, Ricaurte GA, Dannals RF. (1999). Kinetic analysis of [11C]McN5652: a serotonin transporter radioligand. J Cereb Blood Flow Metab.
9 Shank RP, Vaught JL, Pelley KA, Setler PE, McComsey DF, Maryanoff BE. (1988). McN-5652: a highly potent inhibitor of serotonin uptake. J Pharmacol Exp Ther.
10 Ikoma Y, Suhara T, Toyama H, Ichimiya T, Takano A, Sudo Y, Inoue M, Yasuno F, Suzuki K. (2002). Quantitative analysis for estimating binding potential of the brain serotonin transporter with [11 C]McN5652. J Cereb Blood Flow Metab.
11 Suehiro M, Musachio JL, Dannals RF, Mathews WB, Ravert HT, Scheffel U, Wagner HN. (1995). An improved method for the synthesis of radiolabeled McN5652 via thioester precursors. Nucl Med Biol.
12 Suehiro M, Ravert HT, Dannals RF, Scheffel U, Wagner HN. (1992). Synthesis of a radiotracer for studying serotonin uptake sites with positron emission tomography: [11C]McN5652. J. Labelled Compds Radiopharm.
13 Sasaki M, Suhara T, Kubodera A, Suzuki K. (1996). [An improved automated synthesis and in vivo evaluation of PET radioligand for serotonin re-uptake sites: [11C]McN5652X]. Kaku Igaku.
14 Brust P, Zessin J, Kuwabara H, Pawelke B, Kretzschmar M, Hinz R, Bergman J, Eskola O, Solin O, Steinbach J, Johannsen B. (2003). Positron emission tomography imaging of the serotonin transporter in the pig brain using [11C](+)-McN5652 and S-([18F]fluoromethyl)-(+)-McN5652. Synapse.
15 Szabo Z, Scheffel U, Suehiro M, Dannals RF, Kim SE, Ravert HT, Ricaurte GA, Wagner HN. (1995). Positron emission tomography of 5-HT transporter sites in the baboon brain with [11C]McN5652. J Cereb Blood Flow Metab.
16 Laruelle M, Maloteaux JM. (1989). Regional distribution of serotonergic pre- and postsynaptic markers in human brain. Acta Psychiatr Scand Suppl.
17 Kakiuchi T, Tsukada H, Fukumoto D, Nishiyama S. (2001). Effects of aging on serotonin transporter availability and its response to fluvoxamine in the living brain: PET study with [(11)C](+)McN5652 and [(11)C](-)McN5652 in conscious monkeys. Synapse.
18 Szabo Z, Kao PF, Scheffel U, Suehiro M, Mathews WB, Ravert HT, Musachio JL, Marenco S, Kim SE, Ricaurte GA, et al. (1995). Positron emission tomography imaging of serotonin transporters in the human brain using [11C](+)McN5652. Synapse.
19 Reivich M, Amsterdam JD, Brunswick DJ, Shiue CY. (2004). PET brain imaging with [11C](+)McN5652 shows increased serotonin transporter availability in major depression. J Affect Disord.
20 Lammertsma AA, Bench CJ, Hume SP, Osman S, Gunn K, Brooks DJ, Frackowiak RS. (1996). Comparison of methods for analysis of clinical [11C]raclopride studies. J Cereb Blood Flow Metab.
21 Takano A, Suhara T, Sudo Y, Inoue M, Hashimoto K, Zhang MR, Ichimiya T, Yasuno F, Suzuki K. (2002). Comparative evaluation of two serotonin transporter ligands in the human brain: [(11)C](+)McN5652 and [(11)C]cyanoimipramine. Eur J Nucl Med Mol Imaging.
22 Thomasius R, Zapletalova P, Petersen K, Buchert R, Andresen B, Wartberg L, Nebeling B, Schmoldt A. (2006). Mood, cognition and serotonin transporter availability in current and former ecstasy (MDMA) users: the longitudinal perspective. J Psychopharmacol.
23 McCann UD, Szabo Z, Seckin E, Rosenblatt P, Mathews WB, Ravert HT, Dannals RF, Ricaurte GA. (2005). Quantitative PET studies of the serotonin transporter in MDMA users and controls using [11C]McN5652 and [11C]DASB. Neuropsychopharmacology.
24 Buchert R, Thomasius R, Petersen K, Wilke F, Obrocki J, Nebeling B, Wartberg L, Zapletalova P, Clausen M. (2006). Reversibility of ecstasy-induced reduction in serotonin transporter availability in polydrug ecstasy users. Eur J Nucl Med Mol Imaging.
25 Kent JM, Coplan JD, Lombardo I, Hwang DR, Huang Y, Mawlawi O, Van Heertum RL, Slifstein M, Abi-Dargham A, Gorman JM, Laruelle M. (2002). Occupancy of brain serotonin transporters during treatment with paroxetine in patients with social phobia: a positron emission tomography study with 11C McN 5652. Psychopharmacology (Berl).